# [^11^C]2-(2-((Dimethylamino)methyl)phenylthio)-5-(2-fluoroethyl)phenylamine

Chemical name: | [^11^C]2-(2-((Dimethylamino)methyl)phenylthio)-5-(2-fluoroethyl)phenylamine
Abbreviated name: | [^11^C]AFE
Synonym:
Agent Category: | Compound
Target: | Serotonin transporter (SERT)
Target Category: | Ligand binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20AFE%5BAll%20Fields%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

The serotonin neurotransmitter is considered to play an important role in a variety of brain functions such as appetite, sleep, and mood. Neuropsychiatric disorders, including major depression, schizophrenia, and Alzheimer’s and Parkinson’s diseases (1-3), involve a dysfunction of the brain’s serotonin system. The serotonergic neurons – present in wide areas of the brain, including the hypothalamus, thalamus, and cerebral cortex – bear a protein called ”serotonin transporter” (SERT) (4).

The SERT, located on the cell bodies and terminals of 5-hydroxytryptamine (5-HT) neurons, is a specific marker for the number and integrity of presynaptic terminals of serotonin-producing neurons. The SERT regulates neurotransmission by removing released serotonin from the extracellular space back into the presynaptic neuron. Commonly prescribed antidepressants are selective serotonin reuptake inhibitors (SSRIs), and their effect is obtained through interaction with (and inhibition of) the SERT (5). For that reason, in vivo imaging of the regional brain distribution of the SERT is an important tool in the treatment of neuropsychiatric disorders.

A variety of in vivo radioligands for positron emission tomography (PET) have been evaluated for imaging the SERT. [^11^C]McN5652 was the first successful and widely used agent (6, 7), but it does have some limitations because of its slow brain kinetics and low to nonspecific binding ratios in humans. It is adequate for regions with high SERT density but often provides insufficient signal-to-noise differentials for imaging brain regions with intermediate to low SERT densities (e.g., limbic and neocortical regions).

Over recent years, new PET radioligands have been synthesized and evaluated as SERT imaging agents. Among them are ^11^C-labeled N,N-dimethyl-2-(2-amino-4-cyanophenylthio)benzylamine ([^11^C]DASB), 2-(2-(dimethylaminomethyl)phenylthio)-5-fluoromethylphenylamine ([^11^C]AFM), 5-bromo-2-[2-(dimethylaminomethylphenylthio)]phenylamine ([^11^C]DAPA), 2-[2-(dimethylaminomethylphenylthio)]-5-iodophenylamine ([^11^C]ADAM), and N,N-dimethyl-2-(2´-amino-4´-hydroxymethylphenylthio)benzylamine ([^11^C]HOMADAM), which are based on a diaryl sulfide motif (4). [^11^C]2-(2-((Dimethylamino)methyl)phenylthio)-5-(2-fluoroethyl)phenylamine ([^11^C]AFE) has shown a high binding affinity and good selectivity for the SERT and displays signal-to-noise ratios that may enable more reliable mapping of brain regions with low SERT density.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20AFE%5BAll%20Fields%5D%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

[^11^C]AFE can be prepared from its monomethylamino precursor 5-(2-fluoroethyl)-2-(2-((methylamino)methyl)-phenylthio)phenylamine by reaction with either [^11^C]methyl triflate ([^11^C]MeOTf) (8) or [^11^C]MeI, as described by Zhu et al. (9).

In the first method (with [^11^C]MeOTf), the precursor is dissolved in acetone and [^11^C]MeOTf is bubbled through the solution at room temperature. Once maximum activity is reached, the mixture is heated (70 °C for 5 min in a water bath) and purified by high-performance liquid chromatography (HPLC; 40% acetonitrile–60% 0.1 ammonium acetate, pH 6.8). The product is then eluted (~12 min), diluted in 100 ml of H_2_O, loaded on a SepPak, and then eluted with ethanol. The ethanol solution is then mixed with 0.9% sterile saline and filtered through a 0.22 μm membrane to obtain the final product, [^11^C]AFE.

In the second method, [^11^C]AFE is prepared via reaction of the precursor with [^11^C]MeI (trapped at –10 °C). The reaction is performed at 80 °C for 5 min.

The reported radiochemical purity of [^11^C]AFE produced by the first method is >95% (determined by HPLC). The reported radiochemical yields at the end of the synthesis are 32 ± 17% (decay-corrected, based on [^11^C]MeOTf; n = 6) in the first method (8) and 26 ± 14% (decay-corrected, based on [^11^C]MeI; n = 4) in the second method (9). The specific activities of the radiotracer produced are 61,790 ± 32,190 GBq/mmol (1,670 ± 864 Ci/mmol) and 32,079 ± 16,502 GBq/mmol (867 ± 446 Ci/mmol) for the first (8) and second methods (9), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFE%20AND%20in%20vitro)]

The affinities of [^11^C]AFE for the monoamine transporters SERT, dopamine transporter (DAT), and norepinephrine transporter (NET) were determined in vitro by Zhu et al. (9). Experiments were performed with cloned human receptors transfected on HEK-293 cells and the radioligands [^3^H]paroxetine (for SERT), [^3^H]nisoxetine (for NET), and [^3^H]GBR2935 (for DAT). Experiments were performed according to a previously published procedure (10).

[^11^C]AFE displayed a high affinity for SERT (K_i_ = 1.80 ± 0.07 nM), but much lower affinities for NET (K_i_ = 946.2 ± 222.5 nM) and DAT (K_i_ > 10^4^ nM). Additional assays showed that [^11^C]AFE displayed virtually no affinity for benzodiazepine, opioid (μ, σ, and κ) receptors, or for serotonin and dopamine receptors such as 5-HT_1A_, 5-HT_2a_, 5-HT_2c_, 5-HT_3_, 5-HT_6_, 5-HT_7_, and D_1_-D_5_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFE%20AND%20rodentia%5BMeSH%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%22rodentia%22]

Ex vivo biodistribution studies were performed on Sprague-Dawley rats by Zhu et al. (9). The experimental procedure involved injecting 3.7 MBq (100 μCi) of [^11^C]AFE per animal (into the tail vein) and measuring the uptake of the radiotracer at various time points after injection of the radiotracer.

Results showed an overall rapid uptake of [^11^C]AFE into the brain. At 10 min post injection, the measured uptake was 0.8% of the injected dose (ID)/g of tissue. After clearance of the nonspecific binding, [^11^C]AFE showed an uptake pattern consistent with the distribution of SERT in rat brain. The highest levels were found in the hypothalamus, thalamus, frontal cortex, and striatum. The reported specific/nonspecific binding ratios (i.e., ratio of % ID/g in the region of interest to that in the cerebellum) were approximately 5.5 for the hypothalamus and 4.1 for the thalamus at 60 after injection of the tracer.

When pretreated with either cold AFE (2 mg/kg of tissue, given at 10-15 before injection of [^11^C]AFE) or citalopram (an SSRI), 44-62% of the specific binding in the hypothalamus was found to be displaced at 45 min after injection of the tracer. In contrast, pretreatment with nisoxetine (a selective norepinephrine reuptake inhibitor) did not lead to any significant change with respect to [^11^C]AFE-specific binding in SERT-rich regions. Those results indicated that [^11^C]AFE had a high binding selectivity for the SERT.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFE%20AND%20%28pig%20OR%20sheep%20OR%20rabbit%20OR%20dog%29)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%28dog%20OR%20sheep%20OR%20pig%29]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFE%20AND%20%28primate%20NOT%20human%29)]

PET brain imaging studies of 3 male baboons (12 to 32 kg) were performed by Zhu et al. (9) for time periods ranging from 0 to 120 min after administration of [^11^C]AFE (injected dose: approximately 185 MBq (5 mCi); specific activity at time of injection: ~26.7 ± 9.1 GBq/mol (990 ± 338 Ci/mmol); injected mass: 1.66 ± 0.47 μg). The highest levels of the tracer were found in regions of high SERT densities (e.g., thalamus, midbrain, and striatum), and the lowest levels were found in the cerebellum. [^11^C]2-[2-(Dimethylaminomethylphenylthio)]-5-fluorophenylamine ([^11^C]AFA) exhibited rapid uptake kinetics, with activity peaks between 15 and 40 min post injection.

When the baboons were pretreated with 2 mg/kg (4.8 ± 0.5 mCi) of citalopram (an SSRI) 20 min before injection of [^11^C]AFE, the radiotracer uptakes in the midbrain, thalamus, striatum, hippocampus, and cortex were reduced to the level of the cerebellum, showing a significant reduction of the specific binding of [^11^C]AFE in all SERT-containing brain regions. A kinetic analysis done by the authors of the study (9) showed that the regional equilibrium specific-to-nonspecific partition coefficient of [^11^C]AFE was similar to that obtained for the other imaging agent, [^11^C]AFA (with peak uptake occurring between 15 and 40 min after injection of the radiotracer), but lower than those obtained for [^11^C]DASB (e.g., mid-brain: 0.83 ± 0.17, 0.95 ± 0.07, and 1.68 ± 0.23 for [^11^C]AFE, [^11^C]AFA, and [^11^C]DASB respectively). In comparison, the regional equilibrium specific-to-nonspecific partition coefficients for [^11^C]AFM and [^11^C]McN5652 that were reported previously in the literature (11) were 0.94 ± 0.18 ([^11^C]McN5652) and 2.14 ± 0.16 ([^11^C]AFM), respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFE%20AND%20%28human%20NOT%20baboon%29)]

No publication is currently available.

## References

1 Owens MJ Nemeroff CB The serotonin transporter and depression Depress Anxiety 1998 8Suppl 15 12 9809208
2 Palmer AM, Francis PT, Benton JS, Sims NR, Mann DM, Neary D, Snowden JS, Bowen DM. (1987). Presynaptic serotonergic dysfunction in patients with Alzheimer's disease. J Neurochem.
3 Roth BL, Xia Z. (2004). Molecular and cellular mechanisms for the polarized sorting of serotonin receptors: relevance for genesis and treatment of psychosis. Crit Rev Neurobiol.
4 Laakso A, Hietala J. (2000). PET studies of brain monoamine transporters. Curr Pharm Des.
5 White KJ, Walline CC, Barker EL. (2005). Serotonin transporters: implications for antidepressant drug development. Aaps J.
6 Ichimiya T, Suhara T, Sudo Y, Okubo Y, Nakayama K, Nankai M, Inoue M, Yasuno F, Takano A, Maeda J, Shibuya H. (2002). Serotonin transporter binding in patients with mood disorders: a PET study with [11C](+)McN5652. Biol Psychiatry.
7 Suehiro M, Scheffel U, Ravert HT, Dannals RF, Wagner HN. (1993). [11C](+)McN5652 as a radiotracer for imaging serotonin uptake sites with PET. Life Sci.
8 Jewett DM. (1992). A simple synthesis of [11C]methyl triflate. Int J Rad Appl Instrum [A].
9 Zhu Z, Guo N, Narendran R, Erritzoe D, Ekelund J, Hwang DR, Bae SA, Laruelle M, Huang Y. (2004). The new PET imaging agent [11C]AFE is a selective serotonin transporter ligand with fast brain uptake kinetics. Nucl Med Biol.
10 Huang Y, Hwang DR, Zhu Z, Bae SA, Guo N, Sudo Y, Kegeles LS, Laruelle M. (2002). Synthesis and pharmacological characterization of a new PET ligand for the serotonin transporter: [11C]5-bromo-2-[2-(dimethylaminomethylphenylsulfanyl)]phenylamine ([11C]DAPA). Nucl Med Biol.
11 Huang Y, Hwang DR, Narendran R, Sudo Y, Chatterjee R, Bae SA, Mawlawi O, Kegeles LS, Wilson AA, Kung HF, Laruelle M. (2002). Comparative evaluation in nonhuman primates of five PET radiotracers for imaging the serotonin transporters: [11C]McN 5652, [11C]ADAM, [11C]DASB, [11C]DAPA, and [11C]AFM. J Cereb Blood Flow Metab.